# Lys-Thr-Leu-Leu-Pro-Thr-Pro-cross-linked iron oxide-Cy5.5

Chemical name: | Lys-Thr-Leu-Leu-Pro-Thr-Pro-cross-linked iron oxide-Cy5.5
Abbreviated name: | PTP-CLIO-Cy5.5
Synonym:
Agent category: | Peptide
Target: | Plectin-1
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI), optical (near-infrared (NIR) fluorescence)
Source of signal\contrast: | Iron oxide, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=134044255), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=47607491) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5339) for more information about Plectin-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20and%20cy5)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals.

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (3). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal.

A multimodal nanoparticle probe that consists of a contrast agent and a NIR fluorochrome may provide consistent information. CLIO nanoparticles can be internalized by cells of the reticuloendothelial system and have long circulating times in vivo. The blood half-life of CLIO is ~10 h in mice (4). The accumulation of nanoparticles in cells causes a reduction in signal intensity with T2-weighted (T2*W) spin-echo pulse sequences. NIR fluorochromes (e.g., Cy5.5) provide an improved optical (NIR) signal from tissue. CLIO-Cy5.5 has been developed as a multimodal probe for imaging (5).

Patients with pancreatic ductal adenocarcinoma (PDAC) have a median survival of 6 months and a 5-year survival rate of only 3% (6). PDAC is an aggressive cancer with early metastasis in >80% of patients. A method for early detection would be particularly useful for monitoring people at high risk of developing pancreatic cancer. Using phage display screenings, the linear peptide Lys-Thr-Leu-Leu-Pro-Thr-Pro (Plectin-1 targeting peptide, PTP) (7) has been found to specifically bind to Plectin-1, a cytoskeletal protein (8, 9) that is present both inside and on the membrane of human and mouse PDAC cells but only on the inside of normal pancreatic cells. Kelly et al. (7) conjugated PTP to CLIO-Cy5.5 to image Plectin-1 expression in PDAC. PTP-CLIO-Cy5.5 is a multimodal agent that consists of CLIO (MRI) and Cy5.5 (NIR imaging).

### Related Resource Links:

- Chapters in MICAD (Plectin-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Plectin-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (Plectin-1 (http://www.ncbi.nlm.nih.gov/gene/5339)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Plectin-1 (http://www.ncbi.nlm.nih.gov/omim/601282))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20cy5%20and%20synthesis)]

The synthesis of PTP-CLIO-Cy5.5 was described by Kelly et al. (7). The amino-CLIO was labeled with Cy5.5-monofunctional N-hydroxysuccinimide ester to yield CLIO-Cy5.5, which had a diameter of 39 nm as determined with light scattering and R1 and R2 values of 21 and 63 mM^-1^s^-1^, respectively. CLIO-Cy5.5 was purified with column chromatography and reacted with succinimidyl iodoacetic acid for 15 min. PTP-Cys was conjugated with the activated CLIO-Cy5.5 at room temperature for 1 h to yield the multimodal PTP-CLIO-Cy5.5, which had 3.5 PTP molecules and 2.3 Cy5.5 molecules per nanoparticle as determined with spectrophotometry.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20cy5%20and%20in%20vitro)]

Kelly et al. (7) performed cell-binding assays with fluorescein isothiocyanate (FITC)-PTP-phage using human and mouse PDAC cell lines. FITC-PTP-phage and FITC-control phage bound in a similar manner to individual cells with populations of normal human ductal cells. Binding of FITC-PTP-phage to PDAC cells had an average ratio of PTP phage/control phage of 141. Frozen pancreas section studies showed that FITC-PTP-phage bound to PDAC tumor lesions but not to normal regions. Anti–Plectin-1 antibody reduced FITC-PTP-phage binding to PDAC cells by 97%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20cy5%20and%20rodentia)]

Kelly et al. (7) performed biodistribution studies in 9-wk-old Kras/p53^L/+^ mice, which harbor small, focal PDAC as well as regions of normal pancreas, ductal metaplasia, and fibrosis. Intravital confocal microscopy revealed discrete areas of fluorescence in the abdominal region of these mice 24 h after injection of 15 mg Fe/kg PTP-CLIO-Cy5.5. The in vivo fluorescence correlated with surface reflectance imaging of the excised pancreas where discrete foci of signal were found. In contrast, control peptide-CLIO-Cy5.5 failed to highlight any regions of the pancreas. The PDAC tumors accumulated 3.13% of the injected dose at 24 h. Accumulation in the liver was similar to that of the tumors. The kidney, spleen, and lung showed moderate accumulation, and the muscle, intestine, normal pancreas, heart, and skin showed little to minimal accumulation. Control peptide-CLIO-Cy5.5 accumulated 1.9% of the injected dose in the tumors at 24 h with a tissue distribution pattern similar to PTP-CLIO-Cy5.5. Tumor uptake relative to normal pancreas was 10-fold and 4-fold higher for PTP-CLIO-Cy5.5 and control peptide-CLIO-Cy5.5, respectively. MRI showed a reduction in MR signal in focal regions of the pancreas. Histological analysis confirmed that the loss of signal associated with PTP-CLIO-Cy5.5 uptake occurred primarily in PDAC regions but not in normal regions or regions of ductal metaplasia. Fluorescence microscopy of the sections demonstrated PTP nanoparticle accumulation in areas of PDAC but not in areas of normal pancreas. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20cy5%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20cy5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PTP%20CLIO%20cy5%20and%20human)]

No publication is currently available.

## NIH Support

RO1 CA104647, PO1 CA117969, P50 CA86355

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Wunderbaldinger P., Josephson L., Bremer C., Moore A., Weissleder R. (2002). Detection of lymph node metastases by contrast-enhanced MRI in an experimental model. Magn Reson Med.
5 Kircher M.F., Weissleder R., Josephson L. (2004). A dual fluorochrome probe for imaging proteases. Bioconjug Chem.
6 Li D., Xie K., Wolff R., Abbruzzese J.L. (2004). Pancreatic cancer. Lancet.
7 Kelly K.A., Bardeesy N., Anbazhagan R., Gurumurthy S., Berger J., Alencar H., Depinho R.A., Mahmood U., Weissleder R. (2008). Targeted nanoparticles for imaging incipient pancreatic ductal adenocarcinoma. PLoS Med.
8 Andra K., Kornacker I., Jorgl A., Zorer M., Spazierer D., Fuchs P., Fischer I., Wiche G. (2003). Plectin-isoform-specific rescue of hemidesmosomal defects in plectin (-/-) keratinocytes. J Invest Dermatol.
9 Sonnenberg A., Liem R.K. (2007). Plakins in development and disease. Exp Cell Res.